# [^125^I]Anti-claudin 4 monoclonal antibody

Chemical name: | [^125^I]Anti-claudin 4 monoclonal antibody
Abbreviated name: | [^125^I]Anti-claudin 4
Synonym:
Agent Category: | Monoclonal antibody
Target: | Claudin 4 receptor
Target Category: | Antibody-receptor binding
Method of detection: | SPECT, Planar gamma
Source of signal: | ^125^I
Activation: | Not required
Studies: | - Rodents | Click here for Protein and Nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=nuccore&id=34335232) sequence of Claudin 4.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=radiolabeled+anti-claudin+4)]

Claudins are transmembrane proteins that belong to the multigene adhesion molecule family and are found in cellular tight junctions. These proteins are considered to be responsible for the establishment of a paracellular barrier that controls the flow of molecules across the intracellular spaces of the epithelium (1). Claudins are believed to regulate cell proliferation and differentiation because they also bind cell-signaling ligands (2, 3). There are ~24 known claudins that have a tissue-specific expression pattern and any change in their pattern or distribution has been suggested to have a role in the pathology of various disorders, including cancer (4). Gene expression profiling showed that claudin 4, also a receptor for the Clostridium perfringens enterotoxin (5), was overexpressed in pancreatic duct adenocarcinoma, and it is also expressed in normal tissues of the breast, ovaries, prostate, bladder, and gastrointestinal mucosa (6, 7). However, because the level of expression of this protein is significantly higher in primary and metastatic pancreatic cancers, the possible use of claudin 4 as an early marker or therapeutic target for imaging of this cancer was suggested (8).

A mouse anti-claudin 4 monoclonal antibody (https://catalog.invitrogen.com/index.cfm?fuseaction=viewCatalog.viewProductDetails&sku=18-7341&productDescription=10557&orderRequestSource=iGene&ref=) (mAb) is commercially available for in vitro diagnostic use. This mAb was radiolabeled with iodine (^125^I) by Foss et al. (9) for single-photon emission computed tomography–computed tomography (SPECT-CT) imaging of an experimental pancreatic cancer model.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=radiolabeled+anti-claudin+4+antigen+synthesis)]

Preparation of the radiolabeled anti-claudin 4 mouse mAb was described by Foss et al. (9). For this, 20 µg of the mAb in phosphate-buffered saline (PBS; pH 7.5) was dispensed into an iodogen-coated vial and 74–185 MBq (2–5 mCi) ^125^I-labeled sodium iodide in 0.1 M sodium hydroxide (pH 10.0) was added. The solution was mixed and allowed to sit at room temperature for 10 min. At the end of incubation, the labeling solution was loaded onto a desalting column to remove any unincorporated ^125^I.

For use as a negative control, a commercially available mAb against human CD20 (http://www.novusbio.com/data_sheet/index/NB110-7722&prev_module=search) was also labeled with ^125^I following the procedure described above.

The radiochemical yield was reported to be between 30–40% and the radiochemical purity as determined by instant thin-layer chromatography was ≥95%. The investigators did not provide the Rf value of the labeled antibody after ITLC. The specific activities varied from 0.74–1.295 MBq/6.6 pmol (20–35 μCi/6.6 pmol). The labeled antibodies were stored in PBS at 4°C until required and were used within 24 h of labeling.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=radiolabeled+anti-claudin+4+antibody+in+vitro)]

No publications are currently available.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20rodentia)]

The biodistribution of [^125^I]anti-claudin 4 mAb was studied in severe combined immunodeficient (SCID (http://jaxmice.jax.org/library/notes/453a.html)) mice bearing PANC-1 cell xenograft tumors (originating from human exocrine pancreatic carcinoma) (9). SCID mice bearing the PNAC-1 xenografts were injected with the same amount of either the [^125^I]anti-claudin or the [^125^I]anti-CD20 mAb. The mice were euthanized 2, 4, or 6 days after injection and the liver, kidneys, small intestine, bladder, muscle, heart, lungs, stomach, large intestine, spleen, and tumor were removed and weighed to measure the incorporated radioactivity. Among these tissues, the highest uptake of radioactivity was in the liver (4.5% injected dose per gram (ID/g) tissue), the PANC-1 tumors (4% ID/g tissue), and the spleen (3.7% ID/g tissue) 2 days after administration. Radioactivity in the liver was suggested to be a result of the enterohepatic metabolism of the labeled antibody, and uptake by the spleen indicated antibody sequestration in that organ. By comparison, the labeled CD20 antibody was detected during the same period of time primarily in the spleen because white blood cells that express CD20 are stored in this organ. Although some radioactivity was also detected in the liver, the labeled antibody did not exhibit any specificity for the tumors (<0.5% ID/g tissue).

For planar gamma SPECT studies, SCID mice bearing Colo357 cell xenograft tumors (originating from pancreatic carcinoma) were used. Two groups of mice were injected either with the [^125^I]anti-claudin or the [^125^I]anti-CD20 mAb and the animals were subjected to scintigraphy after 2, 4, and 6 days. Mice injected with the [^125^I]anti-claudin 4 antibody showed uptake of the radioactivity primarily in the tumors up to 6 days after the injection. A small amount of label uptake was also evident in the liver and the thyroid during this time. Accumulation of radioactivity in the thyroid was attributed to the dehalogenase activity and release of ^125^I from the anti-claudin 4 antibody. During the same period, animals injected with the [^125^I]anti-CD20 antibody showed accumulation of radioactivity primarily in the spleen and liver (because of antibody metabolism in this organ).

SPECT-CT studies were performed in another group of SCID mice bearing L3.6PL cell pancreatic cancer xenografts (a highly metastatic and aggressive subclone of Colo357 cells). The animals were treated with the [^125^I]anti-claudin mAb and scintigraphy was performed on the animals after 120 h. The tumor and spleen were clearly visible in these animals despite the location of the tumor within the pancreas. The mice were subsequently euthanized and necropsy was performed to determine the amount of radioactivity present in the liver, spleen, and tumor. Measurement of the radioactivity in these organs revealed that the tumor had almost a 2.5-fold higher label uptake compared to the spleen and an approximately 2-fold higher label uptake compared to the liver. No blocking studies that used unlabeled anti-claudin mAb were performed by the investigators.

The investigators suggested that, although the ^125^I-labeled anti-claudin 4 antibody appears to be suitable for SPECT-CT to detect pancreatic cancer, this label is suitable only for imaging small animals with the use of a sensitive gamma camera because of its low-energy gamma photon emission. In the clinic the investigators recommend the use of ^123^I-labeled (for SPECT) or ^124^I-labeled (for positron emission tomography) antibodies to image tumors in patients.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=radiolabeled+anti-claudin+4+antibody+other+non-primate+mammals)]

No publications are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=adiolabeled+anti-claudin+4+antibody++non-human+primates)]

No publications are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=radiolabeled+anti-claudin+4+antibody+human+studies)]

No publications are currently available.

## References

1 Van Itallie C.M., Anderson J.M. (2006). Claudins and epithelial paracellular transport. Annu Rev Physiol.
2 Mitic L.L., Anderson J.M. (1998). Molecular architecture of tight junctions. Annu Rev Physiol.
3 Morin P.J. (2005). Claudin proteins in human cancer: promising new targets for diagnosis and therapy. Cancer Res.
4 Sakai N., Chiba H., Fujita H., Akashi Y., Osanai M., Kojima T., Sawada N. (2007). Expression patterns of claudin family of tight-junction proteins in the mouse prostate. Histochem Cell Biol.
5 Santin A.D., Bellone S., Siegel E.R., McKenney J.K., Thomas M., Roman J.J., Burnett A., Tognon G., Bandiera E., Pecorelli S. (2007). Overexpression of Clostridium perfringens enterotoxin receptors claudin-3 and claudin-4 in uterine carcinosarcomas. Clin Cancer Res.
6 Ryu B., Jones J., Blades N.J., Parmigiani G., Hollingsworth M.A., Hruban R.H., Kern S.E. (2002). Relationships and differentially expressed genes among pancreatic cancers examined by large-scale serial analysis of gene expression. Cancer Res.
7 Rangel L.B., Agarwal R., D'Souza T., Pizer E.S., Alo P.L., Lancaster W.D., Gregoire L., Schwartz D.R., Cho K.R., Morin P.J. (2003). Tight junction proteins claudin-3 and claudin-4 are frequently overexpressed in ovarian cancer but not in ovarian cystadenomas. Clin Cancer Res.
8 Saad R.S., Cho P., Silverman J.F., Liu Y. (2004). Usefulness of Cdx2 in separating mucinous bronchioloalveolar adenocarcinoma of the lung from metastatic mucinous colorectal adenocarcinoma. Am J Clin Pathol.
9 Foss C.A., Fox J.J., Feldmann G., Maitra A., Iacobuzio-Donohue C., Kern S.E., Hruban R., Pomper M.G. (2007). Radiolabeled anti-claudin 4 and anti-prostate stem cell antigen: initial imaging in experimental models of pancreatic cancer. Mol Imaging.